# Gadoversetamide Gd-DTPA-BMEA

Chemical name: | Gadoversetamide | [image]
Abbreviated name: | Gd-DTPA-BMEA | [image]
Synonym: | OptiMARK®, [8,11-bis(carboxymethyl)-14-[2-[(2-methoxyethyl)amno]-2-oxoethyl]-6-oxo-2-oxa-5,8,11,14-tetraazahexadecan-16-oato(3-)] gadolinium | [image]
Backbone: | Compound | [image]
Target: | Nontargeted, central nervous system, liver | [image]
Mechanism: | BBB breakage, liver pathologies with abnormal vascularity | [image]
Method of detection: | Magnetic resonance imaging (MRI) | [image]
Source of contrast/signal: | Gadolinium (Gd) | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Humans | Structure of Gadoversetamide

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=OptiMARK%20or%20gadoversetamide%20or%20Gd-DTPA-BMEA)]

Gadoversetamide (Gd-DTPA-BMEA) is an intravenous, paramagnetic contrast agent of magnetic resonance imaging (MRI) developed for imaging of the central nervous system (CNS) and liver (1, 2). Gadoversetamide is approved by the United States Food and Drug Administration (US FDA) for use with MRI in patients with abnormal blood brain barrier or abnormal vascularity of the brain, spine and associated tissues (3).

Conventional, water-soluble, paramagnetic contrast agents are generally metal chelates with unpaired electrons, and they work by shortening both T_1_ and T_2_ relaxation times of surrounding water protons to produce the contrast-enhancing effect (1, 4-6). At normal clinical doses, the T_1_ effect tends to dominate. Current clinical agents are water-soluble compounds that do not cross the intact blood-brain barrier (BBB).They can be used to enhance signals of CNS tissues that lack a BBB (e.g., pituitary gland), extraaxial tumors (e.g., meningiomas) and areas of BBB breakdown (e.g., tumor margins). In these cases, small or multiple CNS lesions are more clearly delineated with contrast enhancement. In addition, contrast enhancement can highlight vasculature, delineate the extent of disease and confirm the impression of normal or nonmalignant tissues. These contrast agents can also be used in a similar nonspecific manner to enhance contrast between normally perfused areas and pathologies with altered vascularity in the liver (7).

Gadolinium ion (Gd^3+^), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective at enhancing proton relaxation because of its high magnetic moment and very labile water coordination (8-10). Gadopentetate dimeglumine (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar gadolinium chelates have been developed in an effort to further improve clinical efficacy, patient safety and patient tolerance. The major chemical differences among these Gd chelates or Gd-based contrast agents (GBCAs) are the presence or absence of overall charge, ionic or nonionic, and their ligand frameworks (linear or macrocyclic). DTPA-BMEA is a linear nonionic chelate developed as a bis(methoxyethylamide) derivative of DTPA. Being nonionic, Gd-DTPA-BMEA has a lower osmolality of 1110 mOsm/kg (Gd:solute ratio of 1:1) than Gd-DTPA (1940 mOsmo/kg).

The commercial formulation (http://www.imaging.mallinckrodt.com/products/product.asp?ProductID=76) of Gd-DTPA-BMEA contains 330.9 mg of gadoversetamide/ml and has a pH of 5.5-7.5, viscosity of 2.0 cP at 37^o^C, and density of 1.160 g/ml (3)

Both renal and extra-renal toxicities have been reported following the clinical use of gadolinium in patients with underlying kidney disease (11-13). In 2007, the US FDA (http://www.fda.gov/cder/drug/infopage/gcca/default.htm) requested manufacturers of all GBCAs to add new warnings about exposure to GBCAs increases the risk for nephrogenic systemic fibrosis (NSF) in patients with advanced kidney disease.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

DTPA-BMEA was synthesized by reacting the DTPA-bisanhydride with 2-methoxyethylamine at 50^o^C for 4 h as reported by Weber (14, 15). The yield was 93.5%. DTPA-BMEA was then reacted with gadolinium(III) oxide at 60-65^o^C for 3 h to produce Gd-DTPA-BMEA. The final yield was 80.7%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28OptiMARK%20or%20gadoversetamide%20or%20Gd-DTPA-BMEA%29%20AND%20in%20vitro)]

Rothermel and colleagues (14) used radioactive Eu(III) to study the metal exchange kinetics of Gd-DTPA-BMEA in vitro at 0.15 M ionic strength and 25^o^C. They concluded that it had the same dissociative pathways as conventional aminocarboxylate systems, but the incorporation of the two bulky amide groups led to slower rates of formation and dissociation. The in vitro 1/T_1_ nuclear magnetic relaxation dispersion (NMRD) profile of Gd-DTPA-BMEA was assessed in another study (16, 17). The water exchange rate (k_ex_^298^) was found to be 0.39 ± 0.02 x 10^6^ s−^1^ and the activation volume (ΔV≠) was 7.4 ± 0.4 cm^3^ mol−^1^. It also appeared to have a similar 1/T_1_ NMRD profile as Gd-DTPA at 35^o^C. The T_1_ and T_2_ relaxation rates (mM−^1^sec−^1^) in water were reported to be 4.60 and 4.81, respectively

Some studies indicated that Gd-DTPA-BMEA could interfere with in vitro (Ca, Zn, and angiotensin-converting enzyme) colorimetric assays of patient samples (18-20). After continuous exposure to 2500 µg/ml of Gd-DTPA-BMEA in a toxicity study (21), numerical chromosome aberrations in Chinese hamester ovary cells were 5.0% and 3.5% at 24 h and 48 h, respectively. For 5000 µg/ml, the percentages were 6.3% and 22.5%. The results did not support in vivo clastogenic risk for Gd-DTPA-BMEA. Other tests of genetic toxicology (plate incorporation mutagenicity assay and mouse lymphoma mutagenesis assay) were negative.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28OptiMARK%20or%20gadoversetamide%20or%20Gd-DTPA-BMEA%29%20AND%20rodentia)]

The acute LD_50_s for i.v. (mice) and intracisternal (rats) administrations of Gd-DTPA-BMEA were reported to be 25-28 and 0.166 mmol/kg, respectively (21). No repeated-dose toxicity in rats was observed with daily administration of 0.1 mmol/kg for 28 days. Some non-lethal changes were observed with the higher chronic doses of 0.6-3 mmol/kg. In a study of the local tissue toxicity in response to extravascular extravasation, Gd-DTPA-BMEA showed similar reactions, but with less inflammation, as compared with Gd-DTPA (22). The micronucleus cytogenic assay in mice was negative. No effect was observed in reproductive toxicology tests in rats at doses of 0.1-0.7 mmol/kg/day.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28OptiMARK%20or%20gadoversetamide%20or%20Gd-DTPA-BMEA%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

At 0.1 mmol/kg i.v. doses in dogs, Gd-DTPA-BMEA did not appear to cause any toxic or cardiovascular effect (21, 23). At doses of 0.3-1.0 mmol/kg, dose-related decreases in both blood pressure and left ventricular systolic pressure were observed. At higher doses of 0.6-3.0 mmol/kg, abnormal effects were observed in body weights, kidneys, and hematologic parameters. No in utero survival and fetal development effect was observed in rabbits at doses of 0.1-0.4 mmol/kg/day.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28OptiMARK%20or%20gadoversetamide%20or%20Gd-DTPA-BMEA%29%20AND%20human)]

Swan and colleagues (24) conducted a double-blind, randomized, placebo-controlled, parallel-group, multicenter (10 sites) study of 121 subjects who received 0.1-0.5 mmol/kg of Gd-DTPA-BMEA. It was distributed in the extracellular fluid and eliminated primarily in urine, after 72 h, with a mean range from 80% of total excreted activity for the dose of 0.1 mmol/kg to 85% for the dose of 0.5 mmol/kg. This rate appeared to be consistent with renal elimination through glomerular filtration, and elimination was delayed by a decrease in renal function. The normal elimination rate constants (k_el_s) ranged from 0.415 to 0.357 h−^1^ (0.1-0.5 mmol/kg) were decreased to lower rate constants from 0.091 to 0.121 h−^1^ for patients with renal insufficiency. At the doses tested in the study, Gd-DTPA-BMEA appeared to have no adverse effect on kidney function, and no significant changes were observed in patients with CNS or liver pathology. In another study with healthy pediatric subjects (n = 17) who received a single i.v. dose of 0.1 mmol/kg of Gd-DTPA-BMEA, the younger group (from 2 to <5 years of age) had a slight but significantly (P<0.05) shorter mean elimination (t_½_) of 1.19 h than the 1.39 h of the older group (from 5 to <18 years of age) (25).

A 2002 publication summarized the safety data of Gd-DTPA-BMEA from 1663 injections that indicated a similar safety profile with an adverse event ratio (overall adverse events divided by the number of subjects) of 1.95 events/subject as compared with 3.68 events/subject for placebo (n = 46) (26). At the 0.1 mmol/kg i.v. dose of Gd-DTPA-BMEA, the overall adverse event rate was 29.3% (n = 959) and was comparable to 34.7% (n = 329) of Gd-DTPA. Other studies showed that Gd-DTPA-BMEA had a similar clinical efficacy profile when compared with other commercially available MRI contrast agents [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28OptiMARK%20or%20gadoversetamide%20or%20Gd-DTPA-BMEA%29%20AND%20human)].

## Supplemental Information

[Disclaimers]

Gadoversetamide package insert 2007

Gadoversetamide pharmacy bulk package insert

Gadoversetamide material safety data sheet

FDA Information for Healthcare Professionals

## References

1 Baker J.F., Kratz L.C., Stevens G.R., Wible J.H. (2004). Pharmacokinetics and safety of the MRI contrast agent gadoversetamide injection (OptiMARK) in healthy pediatric subjects. Invest Radiol.
2 Brown J.J., Kristy R.M., Stevens G.R., Pierro J.A. (2002). The OptiMARK clinical development program: summary of safety data. J Magn Reson Imaging.
3 OptiMARK (gadoversetamide injection) Packge Insert2007, Tyco Healthcare, Mallinckrodt Inc. p. 1-8.
4 Proctor K.A., Rao L.V., Roberts W.L. (2004). Gadolinium magnetic resonance contrast agents produce analytic interference in multiple serum assays. Am J Clin Pathol.
5 Morawski A.M., Lanza G.A., Wickline S.A. (2005). Targeted contrast agents for magnetic resonance imaging and ultrasound. Curr Opin Biotechnol.
6 Tombach B., Reimer P. (2005). Soluble paramagnetic chelates and stabilized colloidal particle solutions of iron oxides as contrast agents for magnetic resonance imaging. Curr Med Chem.
7 Rubin D., Desser T., Semelka R., Brown J., Nghiem H., Stevens W., Bluemke D., Nelson R., Fultz P., Reimer P., Ho V., Kristy R., Pierro J. (1999). A multicenter, randomized, double-blind study to evaluate the safety, tolerability, and efficacy of OptiMARK (gadoversetamide injection) compared with Magnevist (gadopentetate dimeglumine) in patients with liver pathology: results of a Phase III clinical trial. J Magn Reson Imaging.
8 Tweedle M.F. (1997). The ProHance story: the making of a novel MRI contrast agent. Eur Radiol.
9 Saini, S., and J. T. Ferrucci, Enhanced agents for magnetic resonance imaging: Clinical applications, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 662-681.
10 Desai N.K., Runge V.M. (2003). Contrast use at low field: a review. Top Magn Reson Imaging.
11 Perazella M.A., Rodby R.A. (2007). Gadolinium use in patients with kidney disease: a cause for concern. Semin Dial.
12 Grobner, T. and F.C. Prischl, Gadolinium and nephrogenic systemic fibrosis. Kidney Int, 2007
13 Pedersen M. (2007). Safety update on the possible causal relationship between gadolinium-containing MRI agents and nephrogenic systemic fibrosis. J Magn Reson Imaging.
14 Rothermel G., Rizkalia E., Choppin G. (1997). The kinetics of exchange between a lanthanide ion and the gadolinium complex of N,N"-bis(2-methoxyethylamide-carbamoylmethyl)-diethylenetriamine-N,N',N"-triacetate. Inorg Chim Acta.
15 Weber, R., WeberRW1988, 1988
16 Adzamli K., Periasamy M., Spiller M., Koenig S. (1999). NMRD assessment of Gd-DTPA-bis(methoxyethylamide), (Gd-DTPA-BMEA), a nonionic MRI agent. Invest Radiol.
17 Toth E., Connac F., Helm L., Adzamli K., Merbach A. (1998). 17O-NMR, EPR and NMRD characterization of [Gd(DTPA-BMEA)(H20)]: A neutral MRI contrast agent. Eur J Inorg Chem.
18 Emerson J., Kost G. (2004). Spurious hypocalcemia after Omniscan- or OptiMARK-enhanced magnetic resonance imaging: an algorithm for minimizing a false-positive laboratory value. Arch Pathol Lab Med.
19 Kang H., Scott M., Joe B., Narra V., Heiken J., Parvin C. (2004). Model for predicting the impact of gadolinium on plasma calcium measured by the o-cresolphthalein method. Clin Chem.
20 Proctor K., Rao L., Roberts W. (2004). Gadolinium magnetic resonance contrast agents produce analytic interference in multiple serum assays. Am J Clin Pathol.
21 Wible J., Troup C., Hynes M., Galen K., MacDonald J., Barco S., Wojdyla J., Periasamy M., Adams M. (2001). Toxicological assessment of gadoversetamide injection (OptiMARK), a new contrast-enhancement agent for use in magnetic resonance imaging. Invest Radiol.
22 Runge V., Dickey K., Williams N., Peng X. (2002). Local tissue toxicity in response to extravascular extravasation of magnetic resonance contrast media. Invest Radiol.
23 Wible J.H., Troup C.M., Troup M.R., Hynes K.P., Galen J.R., MacDonald S.J., Barco J.K., Wojdyla M.P., Periasamy M.D., Adams. (2001). Toxicological assessment of gadoversetamide injection (OptiMARK), a new contrast-enhancement agent for use in magnetic resonance imaging. Invest Radiol.
24 Swan S., Baker J., Free R., Tucker R., Barron B., Barr R., Seltzer S., Gazelle G., Maravilla K., Barr W., Stevens G., Lambrecht L., Pierro J. (1999). Pharmacokinetics, safety, and tolerability of gadoversetamide injection (OptiMARK) in subjects with central nervous system or liver pathology and varying degrees of renal function. J Magn Reson Imaging.
25 Baker J., Kratz L., Stevens G., Wible J. (2004). Pharmacokinetics and safety of the MRI contrast agent gadoversetamide injection (OptiMARK) in healthy pediatric subjects. Invest Radiol.
26 Brown J., Kristy R., Stevens G., Pierro J. (2002). The OptiMARK clinical development program: summary of safety data. J Magn Reson Imaging.